# ^177^Lu-CHX-A''-DTPA-ABD-Affibody (Z_HER2:342_)_2_

Chemical name: | ^177^Lu-CHX-A''-DTPA-ABD-Affibody (Z_HER2:342_)_2_
Abbreviated name: | ^177^Lu-ABD-(Z_HER2:342_)_2_
Synonym:
Agent category: | Peptide (macromolecule)
Target: | Human epidermal growth factor receptor (HER2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal/contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=177Lu + her2 + affibody)]

Human epidermal growth factor receptor (HER2, erbB2, neu) is a 185-kDa transmembrane glycoprotein and is a member of the superfamily of epidermal growth factor receptor (EGFR)-type receptor tyrosine kinases (RTKs) (1, 2). HER2 consists of an extracellular domain with four subdomains, a single transmembrane span, a cytoplasmic juxtamembrane linker region, a tyrosine kinase component, and a carboxyl-terminal tail (2). HER2 forms homo-oligomers of itself and heteroligomers with other HER receptors to trigger a complex network of multilayered signal transduction (1), which involves more than 30 ligands and their related adaptor proteins, cascaded enzymes, second messengers, and transcription factors (3). Activation of the network regulates cell growth, cell differentiation, and cell survival. Overexpression of HER2 has been found in a variety of malignant tumors, such as breast cancers (~30% of patients), ovarian cancers, and urinary bladder cancers (4). No ligand that directly binds to HER2 has been clearly identified to date (4). Radionuclide imaging of breast cancers largely relies on radiolabeling of monoclonal antibodies directed against HER2, such as trastuzumab and pertuzumab (5). These antibodies are normally large in size (molecular weight ~150 kDa) and have slow blood clearance and slow tumor penetration, which lead to low contrast in images (6).

Affibody molecules are scaffold proteins that bind to targets with high affinity and specificity (7). Although Affibody molecules are able to bind to the same targets as immunoglobulins, Affibody molecules have no relation to the molecular structures or amino acid sequences of the immunoglobulin family. For example, Z_HER2:342_ (molecular weight ~7 kDa) is an Affibody molecule that specifically targets HER2, which consists of three-helix bundle Z-domains, each formed by 58 cysteine-free amino acids (8). The construction of Z_HER2:342_ is started with a three-helix bundle derived from the immunoglobulin-binding domain (B-domain) of staphylococcal protein A. Then the amino acids on the binding surface are replaced and randomized to remove the original binding affinity and create a completely new binding affinity. The randomization produces a library containing ~10^9^ members, from which Z_HER2:342_ is identified as a ligand with high affinity to HER2 (22 pM). The helix bundle in Z_HER2:342_ provides structural rigidity and conformational stability for efficient binding to the target (9). Affibody molecules can be fused with other proteins/molecules to further modify their affinity/avidity, modulate in vivo kinetics, or introduce a peptide/protein effector function (6).

^177^Lu-CHX-A''-DTPA-ABD-Affibody (Z_HER2:342_)_2_ (^177^Lu-ABD-(Z_HER2:342_)_2_, molecular weight ~19 kDa) is used with single-photon emission computed tomography (SPECT) imaging of HER2 (5). ^177^Lu-ABD-(Z_HER2:342_)_2_ consists of a Z_HER2:342_ dimer, an albumin-binding domain (ABD), and a complex of ^177^Lu-[(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid) (^177^Lu-CHX-A''-DTPA). The use of dimeric Z_HER2:342_ allows for quick extravasation and tumor penetration and stabilizes Z_HER2:342_ binding to HER2 in the presence of ABD. The fused ABD (molecular weight ~5 kDa) is a stable, three-helix bundle of 46 amino acids derived from the monovalent variant of albumin-binding motif in streptococcal protein G (10). ABD binds to albumin in blood reversibly with a dissociation constant of 4 nM (10) to generate a complex of ~87 kDa, leading to a prolonged plasma half-life and reduced uptake in kidneys (5). ^177^Lu is a radionuclide belonging to the group of rare earth radionuclides, and it is produced by neutron bombardment of purified target material in reactors (11). With a half-life of 6.71 days for β^-^ emission at 498 keV and 78% branch fraction, ^177^Lu has been a very promising radionuclide in radiotherapy for effectively destroying small tumors and metastasis (optimal size 1.2–3.0 mm) while sparing normal tissue (12). ^177^Lu also emits low-energy gamma rays at 208 and 113 keV with 10% and 6% abundance, respectively, which allows for direct monitoring of the activity distribution with SPECT and subsequent dosimetry (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + her2 + affibody)+AND+synthesis%0D%0A)]

Tolmachev et al. reported the synthesis of ^177^Lu-ABD-(Z_HER2:342_)_2_ in several steps (5). First, a DNA fragment encoding Z_HER2:342_ was PCR-amplified followed by subcloning in Pseudomonas exotoxin (pET)-derived expression vector pAY540, which contained a gene to encode ABD. Using the restriction enzyme AccI, the molecule was further subcloned in dimeric form to produce a pAy770 vector that encoded a fused ABD (Z_HER2:342_)_2_. pAy770 vector was transformed to chemocompetent Escherichia coli strain BL21(ED3) to express ABD-(Z_HER2:342_)_2_. Then the obtained protein (ABD-(Z_HER2:342_)_2_) with purity >98% was conjugated with the commercial chelator CHX-A''-DTPA at a protein/chelator molar ratio of 1:1 in sodium borate buffer (pH 9.2). Finally, the produced CHX-A''-DTPA-ABD-Affibody (Z_HER2:342_)_2_ was reacted with ^177^Lu salt in acetate buffer (pH 5.5) to produce ^177^Lu-ABD-(Z_HER2:342_)_2_ with labeling efficiency of 88.6%. As determined with liquid chromatographic/mass spectrometry (LC/MS) measurement, ~0.91 chelator was found per ABD-(Z_HER2:342_)_2_ molecule. The dissociation constant of the obtained ^177^Lu-ABD-(Z_HER2:342_)_2_ as measured with the surface plasmon resonance method was 31 nM and 8.2 nM when binding to murine and human albumin, respectively, and 18 pM when binding to the extracellular domain of HER2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177LU + her2 + affibody)+AND+%22in+vitro%22)]

Tolmachev et al. used the surface plasmon resonance method to examine the binding capacity of ^177^Lu-ABD-(Z_HER2:342_)_2_in vitro (5). ^177^Lu-ABD-(Z_HER2:342_)_2_ was added to HER2-expresssing SKOV-3 cells at a ratio of one labeled Affibody dimer per HER2 receptor. After 72 h incubation, the cell radioactivity was measured to evaluate the retention of ^177^Lu-ABD-(Z_HER2:342_)_2_ in the cells. The tissues absorbed ~80% and ~68% of the radioactivity at 8 h and 24 h, respectively, after interrupted incubation. To examine the binding specificity of ^177^Lu-ABD-(Z_HER2:342_)_2_, a 1,000-fold excess of unlabeled Affibody dimer (Z_HER2:342_)_2_ or pertuzumab was added into SKOV-3 cells to saturate HER2 receptors. Then ^177^Lu-ABD-(Z_HER2:342_)_2_ was added 10 min later. Presaturation with (Z_HER2:342_)_2_ almost completely blocked the binding of ^177^Lu-ABD-(Z_HER2:342_)_2_, whereas presaturation with pertuzumab did not reduce the binding at all. These results suggested that ^177^Lu-ABD-(Z_HER2:342_)_2_ and pertuzumab bound to different epitopes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + her2 + affibody) +AND++rodentia)]

The biodistribution of ^177^Lu-ABD-(Z_HER2:342_)_2_ was measured in mice (5). After subcutaneous injection of 1 μg ^177^Lu-ABD-(Z_HER2:342_)_2_ (110 kBq), mice were euthanized at 4, 8, 24, 48, and 72 h (n = 4 for each time point). Blood and tissues were collected for radioactive measurement. At 4 h, the radioactivity (expressed as percent injected activity per gram (% IA/g)) was found to be 5 ± 1 in blood, 1.5 ± 0.4 in lung, 1.0 ± 0.3 in liver, 5.8 ± 0.6 in kidney, and 1 ± 1 in skin. At 24 h, the radioactivity (% IA/g) was 7 ± 0.8 in blood, 3.4 ± 0.4 in lung, 4.1 ± 0.1 in liver, 11 ± 1 in kidney, and 5 ± 3 in skin. At 72 h, the radioactivity (% IA/g) was 3.2 ± 0.3 in blood, 2.2 ± 0.2 in lung, 5 ± 1 in liver, 9 ± 1 in kidney, and 2.6 ± 0.8 in skin. The radioactivity in the blood and kidneys (highest among healthy tissues) peaked at 12 h and 24 h after injection, respectively. The high radioactivity in skin was consistent with the presence of abundant albumin due to relatively large fractional interstitial volume. Compared to the non–albumin-fused analog ^177^Lu-(Z_HER2:342_)_2_, the peak radioactivity of ^177^Lu-ABD-(Z_HER2:342_)_2_ in kidneys was reduced 25-fold; its half-life in the blood also increased from 0.64 ± 0.2 min to 35.8 ± 0.0 min.

The tumor uptake of ^177^Lu-ABD-(Z_HER2:342_)_2_ was examined in nude mice bearing SKOV-3 tumors (5). After subcutaneous injection of 1 μg ^177^Lu-ABD-(Z_HER2:342_)_2_ (110 MBq), mice were euthanized at 1, 4, 12, 48, 168, and 332 h (n = 4 for each time point). The tumor radioactivity (% IA/g) values in the tumor at these time points were 0.13 ± 0.04, 1.9 ± 0.4, 7 ± 4, 19 ± 7, 26 ± 4, 21 ± 6, 9 ± 1, and 1.8 ± 0.2, respectively. The tumor radioactivity concentration of ^177^Lu-ABD-(Z_HER2:342_)_2_ exceeded that in blood and kidney and peaked at 48 h after injection. As a control to examine binding specificity, a group of mice (n = 4) was injected with 1 μg non–HER2-specific Affibody molecule ^177^Lu-ABD-(Z_abeta_)_2_ (110 kBq). The mice were euthanized 48 h after injection; a two-fold reduction of radioactivity was found in blood, and a 9.6-fold reduction was found in the tumor. This suggested that accumulation of ^177^Lu-(Z_HER2:342_)_2_ in tumor primarily depended on its interaction with HER2 but not on unspecific trapping of proteins in tumor interstitium due to higher fractional interstitial volume in tumor tissue. The higher ^177^Lu-ABD-(Z_HER2:342_)_2_ radioactivity found in blood could result from its dissociated portion, which drained from the tumors and then re-entered the blood circulation, whereas such a depot did not exist for ^177^Lu-ABD-(Z_abeta_)_2_. The tumor uptake of ^177^Lu-ABD-(Z_HER2:342_)_2_ was further confirmed with in vivo gamma-camera imaging. At 52 h after injection, prominent accumulation of radioactivity was found in the tumor and in the abdominal area.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + her2 + affibody) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(177Lu + her2 + affibody) +AND+human)]

No publication is currently available.

## References

1 Brennan P.J., Kumagai T., Berezov A., Murali R., Greene M.I. (2000). HER2/neu: mechanisms of dimerization/oligomerization. Oncogene.
2 Landgraf R. (2007). HER2 therapy. HER2 (ERBB2): functional diversity from structurally conserved building blocks. Breast Cancer Res.
3 Zaczek A., Brandt B., Bielawski K.P. (2005). The diverse signaling network of EGFR, HER2, HER3 and HER4 tyrosine kinase receptors and the consequences for therapeutic approaches. Histol Histopathol.
4 Hung M.C. Lau Y.K. Basic science of HER-2/neu: a review Semin Oncol 1999 26Suppl 124 51 9 10482194
5 Tolmachev V., Orlova A., Pehrson R., Galli J., Baastrup B., Andersson K., Sandstrom M., Rosik D., Carlsson J., Lundqvist H., Wennborg A., Nilsson F.Y. (2007). Radionuclide therapy of HER2-positive microxenografts using a 177Lu-labeled HER2-specific Affibody molecule. Cancer Res.
6 Tran T., Engfeldt T., Orlova A., Widstrom C., Bruskin A., Tolmachev V., Karlstrom A.E. (2007). In vivo evaluation of cysteine-based chelators for attachment of 99mTc to tumor-targeting Affibody molecules. Bioconjug Chem.
7 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
8 Tolmachev V., Nilsson F.Y., Widstrom C., Andersson K., Rosik D., Gedda L., Wennborg A., Orlova A. (2006). 111In-benzyl-DTPA-ZHER2:342, an affibody-based conjugate for in vivo imaging of HER2 expression in malignant tumors. J Nucl Med.
9 Tolmachev V., Orlova A., Nilsson F.Y., Feldwisch J., Wennborg A., Abrahmsen L. (2007). Affibody molecules: potential for in vivo imaging of molecular targets for cancer therapy. Expert Opin Biol Ther.
10 Stork R., Muller D., Kontermann R.E. (2007). A novel tri-functional antibody fusion protein with improved pharmacokinetic properties generated by fusing a bispecific single-chain diabody with an albumin-binding domain from streptococcal protein G. Protein Eng Des Sel.
11 Schotzig U., Schrader H., Schonfeld E., Gunther E., Klein R. (2001). Standardisation and decay data of 177Lu and 188Re. Appl Radiat Isot.
12 Dvorakova Z., Henkelmann R., Lin X., Turler A., Gerstenberg H. (2008). Production of 177Lu at the new research reactor FRM-II: Irradiation yield of 176Lu(n,gamma)177Lu. Appl Radiat Isot.